# N2-{6-[(4-Amino-6,7-dimethoxy-2-quinazolinyl)(methyl)amino]hexyl}-N2-[^11^C]methyl-2-furamide

Chemical name: | N2-{6-[(4-Amino-6,7-dimethoxy-2-quinazolinyl)(methyl)amino]hexyl}-N2-[^11^C]methyl-2-furamide
Abbreviated name: | [^11^C]GB67
Synonym:
Agent category: | Compound
Target: | α_1_-Adrenoceptor
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20GB67)]

Malfunction of the sympathetic nervous system may play a primary role in the pathogenesis of heart diseases. There are two subtypes of α-adrenoceptors: α_1_ and α_2_ in the heart. α-Adrenoceptors play a backup role for β_1_-adrenoceptors (1). The cardiac adrenoceptors are responsible for the regulation of heart rate and myocardial contractility (2). About 15% of cardiac adrenoceptors are made up of α_1_-adrenoceptors. Presynaptic α_1_-adrenoceptors modulate noradrenalin release. α_1_-Adrenoceptors are present predominately in larger blood vessels, whereas α_2_-adrenoceptors are more prominent in smaller blood vessels. Increases in α_1_-adrenoceptor sites are usually observed when the number of β-adrenoceptors decreases in heart diseases (3). Imaging of the pathologic changes of adrenergic receptors offers a non-invasive assessment of myocardial diseases.

N2-{6-[(4-Amino-6,7-dimethoxy-2-quinazolinyl)(methyl)amino]hexyl}-N2-methyl-2-furamide (GB67) was reported to be a structural and pharmacologic analog of the α_1_-adrenoceptor antagonist prazosin (an antihypertensive agent) (4). GB67 exhibited high potency and selectivity for α_1_-adrenoceptors. [^11^C]GB67 is being developed as a positron emission tomography (PET) agent for use in non-invasive study of α_1_-adrenoceptors in the heart.

### Related Resource Links:

- Chapters in MICAD (Adrenoceptors (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=adrenoceptors%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (α_1_-adrenoceptors (http://www.ncbi.nlm.nih.gov/gene?term=alpha%20adrenoceptor%20human), α_2_-adrenoceptors (http://www.ncbi.nlm.nih.gov/gene?term=alpha%20adrenoceptor%20human))
- Articles in OMIM (α_1_-adrenoceptors (http://omim.org/search?index=entry&start=1&limit=10&search=alpha-1-adrenergic+receptor&sort=score+desc+%2C+prefix_sort+desc&sort=score+desc+%2C+prefix_sort+desc), α_2_-adrenoceptors (http://omim.org/search?index=entry&start=1&limit=10&search=alpha-2-adrenergic+receptor&sort=score+desc+%2C+prefix_sort+desc&sort=score+desc+%2C+prefix_sort+desc))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20GB67%20and%20synthesis)]

[^11^C]GB67 was synthesized remotely via a one-pot reaction of [^11^C]methyl iodine with desmethyl precursor (N2-{6-[(4-amino-6,7-dimethoxy-2-quinazolinyl)(methyl)amino]hexyl}-2-furamide or N-desmethylamido-GB67) in the presence of NaH. [^11^C]GB67 was purified by high-performance liquid chromatography (HPLC) with a radiochemical yield of 18% (end of bombardment) (5). The radiochemical purity was >99%, and the specific activity was 20-60 GBq/μmol (0.54-1.62 Ci/μmol) at end of synthesis. Time of synthesis was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20GB67%20and%20in%20vitro)]

In vitro competition binding studies of [^3^H]prazosin with human heart membranes produced a K_d_ of 0.9 ± 0.08 nM and a B_max_ of 58 ± 5 fmol/mg protein (6). In the rat heart membranes, the K_d_ and B_max_ were reported to be 0.23 ± 0.04 nM and 63 ± 0.04 fmol/mg protein, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20GB67%20and%20rodentia)]

Law et al. (5) performed biodistribution studies in normal rats and found high accumulation of radioactivity in the kidney (tissue/plasma ratio of 42), followed by the liver (37), lung (25), heart (29), and muscle (2) at 60 min after injection of 0.4-0.8 nmol/kg [^11^C]GB67. Radioactivity in the brain was very low (tissue/plasma ratio of 0.5). Pretreatment of rats with unlabeled GB67 (0.1 or 5 μmol/kg) significantly decreased the accumulation of [^11^C]GB67 in the heart but not in the other tissues. Co-injection of 1-100 nmol/kg GB67 decreased the accumulation in the myocardium in a dose-dependent manner. Injection of unlabeled prazosin (100 nmol/kg) 5 min after injection of [^11^C]GB67 produced significant displacement of radioactivity from the myocardium at 20 min after injection of the tracer. Rx 821002 (α_2_-adrenoceptors) and CGP 12177 (β-adrenoceptors) at 5 μmol/kg had no effect on blocking [^11^C]GB67 accumulation in the heart, indicating α_1_-adrenoceptor selectivity for [^11^C]GB67. In a competitive binding model, the B_max_ and K_d_ for the myocardium were estimated to be 13 pmol/g tissue and 1.5 nmol/kg of body weight, respectively. Almost all of the radioactivity in the heart was intact [^11^C]GB67 at 60 min post injection. The fraction of unchanged [^11^C]GB67 in blood, as determined by HPLC, was 82% at 5 min and 54% at 25 min.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20GB67%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

PET studies (n = 7) were performed in pigs. [^11^C]GB67 volume of distribution (V_T_) values (in ml cm^-3^) were estimated to be 24.2 ± 5.5 (range, 17.3-31.3), 10.1 (predose) and 11.6 (displacement). MBF did not differ within each pig, including between baseline and predose conditions. Predose and displacement studies showed that specific binding of [^11^C]GB67 to myocardial α_1_-adrenoceptors accounts for ~50% of V_T_.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20GB67%20and%20%28primate%20not%20human%29)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20GB67%20and%20human)]

Law et al. (5) reported a human PET study in which [^11^C]GB67 (153.2-384.5 MBq (4.1-10.4 mCi)) was administered to 2 healthy male volunteers. The myocardium was clearly visualized early, and the retention of radioactivity remained unchanged up to 60 min. On the other hand, radioactivity in the lung decreased rapidly. The fraction of unchanged [^11^C]GB67 in blood, as determined by HPLC, was 96% at 5 min and 82% at 25 min.

## References

1 Heusch G. (1990). Alpha-adrenergic mechanisms in myocardial ischemia. Circulation.
2 Brodde O.E. (1991). Beta 1- and beta 2-adrenoceptors in the human heart: properties, function, and alterations in chronic heart failure. Pharmacol Rev.
3 Bristow M.R., Minobe W., Rasmussen R., Larrabee P., Skerl L., Klein J.W., Anderson F.L., Murray J., Mestroni L., Karwande S.V., et al. (1992). Beta-adrenergic neuroeffector abnormalities in the failing human heart are produced by local rather than systemic mechanisms. J Clin Invest.
4 Giardina D., Gulini U., Massi M., Piloni M.G., Pompei P., Rafaiani G., Melchiorre C. (1993). Structure-activity relationships in prazosin-related compounds. 2. Role of the piperazine ring on alpha-blocking activity. J Med Chem.
5 Law M.P., Osman S., Pike V.W., Davenport R.J., Cunningham V.J., Rimoldi O., Rhodes C.G., Giardina D., Camici P.G. (2000). Evaluation of [11C]GB67, a novel radioligand for imaging myocardial alpha 1-adrenoceptors with positron emission tomography. Eur J Nucl Med.
6 Fedida D., Braun A.P., Giles W.R. (1993). Alpha 1-adrenoceptors in myocardium: functional aspects and transmembrane signaling mechanisms. Physiol Rev.